# Cy5.5 conjugated anti-epidermal growth factor receptor monoclonal antibody

Chemical name: | Cy5.5 conjugated anti-epidermal growth factor receptor monoclonal antibody
Abbreviated name: | Cetuximab-Cy5.5
Synonym:
Agent Category: | Anti-epidermal growth factor receptor monoclonal antibody
Target: | Epidermal growth factor receptor
Target Category: | Antibody-ligand binding
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click here for nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=158936071) and protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=110002567) sequence of human EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cetuximab-Cy5.5)]

The epidermal growth factor receptor (EGFR) is a 170-kDa transmembrane protein that promotes cell proliferation by the specific binding of the autocrine epidermal growth factor (EGF) and transforming growth factor α (TGFα). The activity of these factors is believed to contribute to the progression of cancers. The EGFR operates through a receptor-associated tyrosine kinase–mediated signal transduction pathway that triggers cell proliferation. Overexpression of the EGFR is a characteristic feature of a variety of cancers such as squamous cell lung carcinoma and breast, ovarian, head and neck, bladder, and colon cancers (1). Much evidence indicates, in addition to overexpression, that a mutated EGFR gene may play a role in the development of these cancers (2). The most common mutation results in the development of a truncated receptor gene (EGFRvIII) that is deficient in exons 2–7 of the coding sequence. The mutant gene produces a receptor that lacks a part of the extracellular ligand-binding domain that is not activated by ligand binding. However, the intracellular tyrosine kinase portion of the receptor is constitutively active and autophosphorylates the tyrosine residue that initiates the signaling pathway for cell proliferation. In an effort to develop cancer therapies, a variety of EGFR inhibitors have been developed that either inhibit activation of the receptor kinase or the receptor binding of EGF and TGFα, e.g., monoclonal antibodies (mAbs) to the receptor (3, 4).

Cetuximab is a human chimeric anti-EGFR mAb that has been successfully used by itself and in combination with chemo- and radiation therapy for the treatment of solid tumors or metastasized cancers (5, 6). Cetuximab is available commercially in the United States and has been approved (http://www.cancer.gov/cancertopics/druginfo/cetuximab) by the United States Food and Drug Administration for the treatment of metastasized colorectal cancer and advanced squamous cell carcinoma of the head and neck. It is currently being evaluated in several clinical trials (http://www.cancer.gov/search/ResultsClinicalTrialsAdvanced.aspx?protocolsearchid=2740900) for the treatment of a variety of cancers. Because of EGFR heterogeneity in cancers, the imaging of cetuximab binding could assist in the selection and treatment of patients who are likely to respond to treatment and enhance the possibility of a positive outcome of the therapy. Radiolabeled cetuximab has been used to visualize and monitor EGFR tumors in animals and humans (7-10).

In an effort to develop a non-radiolabeled imaging agent for EGFR, cetuximab was labeled with Oregon Green 488 (OG), a fluorescent dye, for the in vitro and in vivo visualization of EGFR in tumor tissue (11). Surgical resection is often an option to treat patients with cancerous tumors, but during surgery it is not possible to distinguish between the neoplastic tissue and the surrounding normal tissue, and some cancerous cells may be left behind, which may lead to relapse of the cancer. Recently, cetuximab was conjugated with Cy5.5, another fluorescent dye, to evaluate the use of a fluorescent dye–conjugated antibody to detect any residual cancerous cells after tumor resection of head and neck squamous cell carcinoma xenografts in mice (12-14)..

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cetuximab-Cy5.5+synthesis)]

The synthesis of cetuximab-Cy5.5 was described by Rosenthal et al. (13). Cetuximab (http://erbitux.com/erbitux/erb/patient_crc/channels/content.jsp?BV_UseBVCookie=Yes&channelId=-88702&gclid=CMy9wbePmY8CFQSNHgodgXjKTQ) and Cy5.5 (http://www4.gelifesciences.com/aptrix/upp00919.nsf/Content/471D8B77EC56CD5FC1256EB400418063/$file/PA25500PS+Rev-D,+2003.pdf)-reactive dye were obtained commercially. Cetuximab was incubated with the Cy5.5-reactive dye in 0.15 M phosphate buffer at pH 7.8 for 1.5 h. Excess dye was removed by centrifugation from the conjugated mAb. The purity of the fluorescent mAb and the number of dye molecules conjugated per molecule of the mAb were not provided by the investigators.

Commercially available non-specific human immunoglobulin IgG1k antibody was also labeled with Cy5.5 as described above for use as a control (13).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cetuximab-Cy5.5+in+vitro)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cetuximab-Cy5.5+rodentia)]

Mice bearing orthotopically xenografted human neck squamous cell carcinoma (HNSCC) cell line (SCC1, CAL27, and FaDu) tumors were used to evaluate the use of cetuximab-Cy5.5 for the optical visualization of neoplastic tissue (13). Two animals for each group (IgG1k-Cy5.5 and cetuximab-Cy5.5) for each cell line were treated. The conjugated antibodies were administered to the animals through the tail vein, and optical imaging was performed between 0 and 72 h after the injection. Surgical resections were performed on the animals after they were killed, and stereomicroscopic imaging was performed before and after each partial or near-total surgical resection. Hematoxylin-eosin staining was also performed on serial histological sections to assess the location of any residual tumor. All the xenografted tumors showed higher fluorescence with cetuximab-Cy5.5 compared to the almost background levels observed with IgG1k-Cy5.5 (13).

After surgical resection of tumors visualized by fluorescence, the mandible and attached structures were removed, embedded in paraffin, and serially sectioned in the axial plane (13). Hematoxylin-eosin staining of the histological sections confirmed the presence of tumors previously identified by fluorescence. The investigators concluded that this imaging technique has potential use for the detection and visualization of HNSCC for pre-, intra-, and post-operative procedures.

In another study from the same laboratory, the investigators evaluated the visualization of human tumor cell line xenografts (same as above), transplanted human tumor xenografts, and mouse mesothelioma tumors with cetuximab-Cy5.5 (14). In this study, IgG1k-Cy5.5 was again used as a control antibody. The mice were injected with cetuximab-Cy5.5 or the control antibody as before, and the tumors were visualized with time-domain fluorescence imaging or fluorescence stereomicroscopy. The investigators observed significantly higher fluorescence over background from tumors of mice treated with cetuximab-Cy5.5 between 6 and 24 h after the conjugated antibody injection. This study confirmed the earlier observations made by the investigators (13).

To simulate clinical use of the Cy5.5-conjugated cetuximab, SCC-1 flank tumors in the mice underwent partial and full resection from the animals (14). Imaging with Cy5.5 fluorescent stereomicroscopy revealed any residual tumor in animals with partially removed tumors. Fluorescent imaging did not reveal any tumors in animals that had undergone complete removal of the xenograft tumors. From this study it was concluded that fluorescent imaging can be used to obtain real-time information for surgical resection of cancerous tumors (14).

Using a subcutaneous flank (n=18) and an orthotropic (n=15) murine model, Kulbersh et al. compared the sensitivity and specificity of optical fluorescence imaging to that of a histopathological evaluation of SCC-1 xenografted tumors in mice (12). In the subcutaneous flank model, a diagnostic dose of 322.5 pmol and a therapeutic dose of 1.61 nmol of cetuximab-Cy5.5 were respectively administered to the animals. With this model, although both doses had a specificity of 100%, the sensitivity was 86% and 91% for the diagnostic and therapeutic doses, respectively (12). For the orthotropic model, only the diagnostic dose was used and the sensitivity and specificity were determined to be 81% and 100%, respectively. The investigators also observed that false-negative results were obtained from tumors measuring <0.5 mm in diameter with the orthotropic model. From these results it was concluded that the use of a fluorescently labeled anti-EFGR antibody to detect disease should be further evaluated before use in humans.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cetuximab-Cy5.5+Non-Primate+Mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cetuximab-Cy5.5+Non-Human+Primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cetuximab-Cy5.5+Human+Studies)]

No publications are currently available.

## References

1 Gullick W.J. (1991). Prevalence of aberrant expression of the epidermal growth factor receptor in human cancers. Br Med Bull.
2 Sok J.C., Coppelli F.M., Thomas S.M., Lango M.N., Xi S., Hunt J.L., Freilino M.L., Graner M.W., Wikstrand C.J., Bigner D.D., Gooding W.E., Furnari F.B., Grandis J.R. (2006). Mutant epidermal growth factor receptor (EGFRvIII) contributes to head and neck cancer growth and resistance to EGFR targeting. Clin Cancer Res.
3 Dancey J.E. (2003). Recent advances of molecular targeted agents: opportunities for imaging. Cancer Biol Ther.
4 Dancey J.E., Freidlin B. (2003). Targeting epidermal growth factor receptor--are we missing the mark?. Lancet.
5 Bonner J.A., Harari P.M., Giralt J., Azarnia N., Shin D.M., Cohen R.B., Jones C.U., Sur R., Raben D., Jassem J., Ove R., Kies M.S., Baselga J., Youssoufian H., Amellal N., Rowinsky E.K., Ang K.K. (2006). Radiotherapy plus cetuximab for squamous-cell carcinoma of the head and neck. N Engl J Med.
6 Xiong H.Q., Rosenberg A., LoBuglio A., Schmidt W., Wolff R.A., Deutsch J., Needle M., Abbruzzese J.L. (2004). Cetuximab, a monoclonal antibody targeting the epidermal growth factor receptor, in combination with gemcitabine for advanced pancreatic cancer: a multicenter phase II Trial. J Clin Oncol.
7 Cai W., Chen K., He L., Cao Q., Koong A., Chen X. (2007). Quantitative PET of EGFR expression in xenograft-bearing mice using (64)Cu-labeled cetuximab, a chimeric anti-EGFR monoclonal antibody. Eur J Nucl Med Mol Imaging.
8. Pantaleo, M.A., S. Fanti, P.L. Lollini, S. Boschi, and G. Biasco, PET detection of epidermal growth factor receptor in colorectal cancer: a real predictor of response to cetuximab treatment? Eur J Nucl Med Mol Imaging, 2007.
9 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
10 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
11 Aerts H.J., Dubois L., Hackeng T.M., Straathof R., Chiu R.K., Lieuwes N.G., Jutten B., Weppler S.A., Lammering G., Wouters B.G., Lambin P. (2007). Development and evaluation of a cetuximab-based imaging probe to target EGFR and EGFRvIII. Radiother Oncol.
12 Kulbersh B.D., Duncan R.D., Magnuson J.S., Skipper J.B., Zinn K., Rosenthal E.L. (2007). Sensitivity and specificity of fluorescent immunoguided neoplasm detection in head and neck cancer xenografts. Arch Otolaryngol Head Neck Surg.
13 Rosenthal E.L., Kulbersh B.D., Duncan R.D., Zhang W., Magnuson J.S., Carroll W.R., Zinn K. (2006). In vivo detection of head and neck cancer orthotopic xenografts by immunofluorescence. Laryngoscope.
14 Rosenthal E.L., Kulbersh B.D., King T., Chaudhuri T.R., Zinn K.R. (2007). Use of fluorescent labeled anti-epidermal growth factor receptor antibody to image head and neck squamous cell carcinoma xenografts. Mol Cancer Ther.